# ^18^F-1,4,7-Triazacyclononane-1,4,7-triacetic acid-10-maleimidoethylacetamide-Affibody Z_HER2:2395_

Chemical name: | ^18^F-1,4,7-Triazacyclononane-1,4,7-triacetic acid-10-maleimidoethylacetamide-Affibody Z_HER2:2395_
Abbreviated name: | ^18^F-NOTA-Z_HER2:2395_
Synonym: | ^18^F-[MMA-NOTA-Cys^61^]-Z_HER2:2395_
Agent category: | Antibody fragment, Affibody
Target: | Epidermal growth factor receptor-2 (EGFR-2, HER2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395)]

Epidermal growth factor (EGF) is a cytokine composed of 53 amino acids (6.2 kDa), and it is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on the 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A cysteine molecule was introduced at the C-terminus of Affibody molecules for site-specific coupling with the chelator 1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidoethylacetamide (MMA-DOTA) for ^111^In labeling. ^111^In-[MMA-DOTA-Cys^61^]-Z_HER2:2395_ (^111^In-DOTA-Z_HER2:2395_ (http://www.ncbi.nlm.nih.gov/books/NBK23711/#Z-2395-DOTA-111In)) has been evaluated in nude mice bearing human colon adenocarcinoma tumors (18). Heskamp et al. (19) prepared ^18^F-1,4,7-triazacyclononane-1,4,7-triacetic acid-10-maleimidoethylacetamide-Affibody Z_HER2:2395_ (^18^F-NOTA-Z_HER2:2395_) by complexation of Al^18^F with NOTA as a positron emission tomography (PET) agent for imaging HER2 expression.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20synthesis)]

Affibody Z_HER2:2395_ was reduced with dithiothreitol in 0.02 M ascorbic acid for 18 h at 37°C (19). The reduced Z_HER2:2395_ was incubated with MMA-NOTA in 1:3 molar ratio in ammonium acetate buffer (pH, 5.5) for 1 h at 37°C. NOTA-Z_HER2:2395_ was isolated with high-performance liquid chromatography. There was one NOTA moiety per NOTA-Z_HER2:2395._ NOTA-Z_HER2:2395_ (~40 nmol) was mixed with ~60 MBq (1.6 mCi) Al^18^F and incubated for 15 min at 90°C. The labeling efficiency of ^18^F incorporation was 21%. ^18^F-NOTA-Z_HER2:2395_ was isolated with column chromatography with >95% radiochemical purity. Specific activity of the preparation was 7.7 GBq/µmol (208 mCi/µmol) at the end of synthesis. ^18^F-NOTA-Z_HER2:2395_ remained intact after incubation in human or mouse serum for 4 h at 37°C. ^111^In-NOTA-Z_HER2:2395_ and ^68^Ga-NOTA-Z_HER2:2395_ were also prepared, with specific activities of 22.4 GBq/µmol (605 mCi/µmol) and 39.6 GBq/µmol (1,070 mCi/µmol) at the end of synthesis, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20in%20vitro)]

Ahlgren et al. (18) performed binding experiments with Z_HER2:2395_ with the use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_d_ value of Z_HER2:2395_ was calculated to be 27 pM. The K_d_ value of Z_HER2:342_ was 22 pM. Hence, the binding affinity of Z_HER2:2395_ was the same as the parent Affibody molecule Z_HER2:342_. In vitro binding specificity tests showed that binding of Z_HER2:2395_ to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^111^In-DOTA-Z_HER2:2395_.

Heskamp et al. (19) performed in vitro binding assays of ^18^F-NOTA-Z_HER2:2395_ to SKOV-3 cells. ^18^F-NOTA-Z_HER2:2395_ exhibited a K_d_ value of 6.5 ± 1.2 nM and 1.3 ± 0.4 × 10^6^ binding sites/cell. ^nat^F-NOTA-Z_HER2:2395_, ^nat^In-NOTA-Z_HER2:2395_, and ^nat^Ga-NOTA-Z_HER2:2395_ exhibited IC_50_ values of 5.0 ± 0.1, 6.3 ± 0.1, and 5.1 ± 0.1 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20rodentia)]

Heskamp et al. (19) performed ex vivo biodistribution studies with 1 MBq (27 μCi) ^18^F-NOTA-Z_HER2:2395_, 0.4 MBq (11 μCi) ^111^In-NOTA-Z_HER2:2395_, and 5 MBq (135 μCi) ^68^Ga-NOTA-Z_HER2:2395_ in nude mice (n = 6/group) bearing SKOV-3 xenografts. The amount of each tracer injected intravenously to each mouse was ~1.6 nmol. The tumor accumulation of radioactivity at 1 h after injection was 4.4 ± 0.8% injected dose/gram (ID/g), 5.6 ± 1.6%, and 7.1 ± 1.4% for ^18^F-NOTA-Z_HER2:2395_, ^68^Ga-NOTA-Z_HER2:2395_, and ^111^In-NOTA-Z_HER2:2395_, respectively. The radioactivity level in tumors was higher than in other organs and tissues (the lung, liver, spleen, and intestines) except the kidneys (~140% ID/g). The biodistribution was characterized by quick clearance of radioactivity from blood and normal organs except the kidneys. The tumor/blood ratios were 7.4, 8.0, and 4.8 for ^18^F-NOTA-Z_HER2:2395_, ^68^Ga-NOTA-Z_HER2:2395_, and ^111^In-NOTA-Z_HER2:2395_, respectively. At 4 h after injection, the tumor/blood ratios were 145 and 42 for ^18^F-NOTA-Z_HER2:2395_ and ^111^In-NOTA-Z_HER2:2395_, respectively. Co-administration of excess Z_HER2:342_ decreased tumor accumulation of the three tracers by ~60% (P = 0.05) at 1 h after injection. Little reduction was observed in the other organs.

PET analysis was performed in nude mice bearing the SKOV-3 tumors at 1 h and 4 h after injection (19). The tumors were clearly visualized along with the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Ahlgren S., Orlova A., Rosik D., Sandstrom M., Sjoberg A., Baastrup B., Widmark O., Fant G., Feldwisch J., Tolmachev V. (2008). Evaluation of maleimide derivative of DOTA for site-specific labeling of recombinant affibody molecules. Bioconjug Chem.
19 Heskamp S., Laverman P., Rosik D., Boschetti F., van der Graaf W.T., Oyen W.J., van Laarhoven H.W., Tolmachev V., Boerman O.C. (2012). Imaging of Human Epidermal Growth Factor Receptor Type 2 Expression with 18F-Labeled Affibody Molecule ZHER2:2395 in a Mouse Model for Ovarian Cancer. J Nucl Med.